# ^89^Zr-Labeled fresolimumab (human anti-transforming growth factor-β monoclonal antibody)

Chemical name: | ^89^Zr-Labeled fresolimumab (human anti-transforming growth factor-β monoclonal antibody)
Abbreviated name: | [^89^Zr]-Fresolimumab
Synonym: | GC1008 (produced by Genzyme)
Agent Category: | Antibody
Target: | Transforming growth factor-β
Target Category: | Antigen
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^89^Zr
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=tgf%20beta%20review&cmd=DetailsSearch)]

The transforming growth factor-β (TGF-β) belongs to a superfamily of cytokines that mediate their activity through serine/threonine kinase receptors and are involved in a variety of cellular processes such as proliferation, differentiation, and migration (1, 2). The TGF-β is a tumor suppressor, but under certain cellular conditions it can promote tumor progression and cancer metastasis as discussed by Meulmeester and ten Dijke (2) and Inman (3). Although TGF-β and its receptors are considered to be important targets for the treatment of highly invasive tumors such as glioblastomas (http://www.cedars-sinai.edu/Patients/Health-Conditions/Glioblastoma-Multiforme-Brain-Tumors.aspx) and those of breast cancer (http://www.cedars-sinai.edu/Patients/Health-Conditions/Breast-Cancer.aspx), no drug or antibody is available to inhibit the activity of this cytokine or its receptor signaling pathway to treat these malignancies (4). A subset of breast cancer patients exhibited overexpression or suppression of genes related to the TGF-β signaling pathway, and these individuals also showed a shorter metastasis-free or relapse-free survival (5). Therefore, noninvasive imaging of TGF-β will not only help in understanding the functioning of this receptor–ligand system and assist in the development of novel agents that can target the TGF-β or its receptor, but it will also assist in the selection of patients who would benefit most from such an anti-cancer treatment (5).

Fresolimumab, a human anti-TGF-β monoclonal antibody (mAb) that neutralizes all active isoforms of TGF-β, was developed and used in a phase I study for the treatment of 22 patients with advanced melanoma and renal cell carcinoma (5). After the treatment, one patient showed stable disease, one patient had a partial response, and three patients showed a mixed response. In addition, no dose-limiting toxicity with the Ab was apparent in the patients. To further improve the likelihood of a positive outcome after the treatment with fresolimumab, it would be helpful to know if the TGF-β or its receptor are overexpressed and activated in the tumor, and also whether the mAb is able to detect such tumors. For this, Oude Munnink et al. evaluated ^89^Zr-labeled fresolimumab ([^89^Zr]-fresolimumab) for the detection and quantification of tumors that overexpress TGF-β with positron emission tomography (PET) in a nude mouse model (5). The investigators chose to label the mAb with ^89^Zr because it has a long half-life (~78 h), and is also suitable to study binding of the labeled antibody to the tumor and to monitor its organ distribution in animal models. The biodistribution of [^89^Zr]-fresolimumab was also studied in mice bearing xenograft tumors that express varying levels of TGF-β.

### Related Resource Links

mRNA and Protein (http://www.ncbi.nlm.nih.gov/nuccore/1813326?report=genbank) sequence of TGF-β (GenBank )

TGF-β in Online Mendelian Inheritance in Man Database (OMIM) (http://omim.org/entry/190180)

TGF-β receptor signaling in Pathway Interaction Database (http://pid.nci.nih.gov/search/pathway_landing.shtml?pathway_id=tgfbrpathway&pathway_name=TGF-beta%20receptor%20signaling&source=NCI-Nature%20curated&what=graphic&jpg=on&ppage=1)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Transforming+growth+factor) related to TGF-β

TGF-β and cancer therapy [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=TGF%20beta%20and%20cancer%20therapy&cmd=DetailsSearch)]

Diseases related to TGF- β (http://www.kegg.jp/kegg-bin/search_result?db=disease&lang=&pid=13275085694153&q=TGF%20beta&show=pathway) (From Kyoto Encyclopedia of Genes and Genomics)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-fresolimumab%20synthesis&cmd=DetailsSearch)]

Fresolimumab was obtained from a commercial source and conjugated with N-succinyldesferrioxamine-B-tetrafluorphenol (N-sucDf-TFP) as detailed by Oude Munnink et al. (5). Fresolimumab and N-sucDf-TFP had an effective conjugation of 62.0 ± 9.0%. N-sucDf-fresolimumab was stored at −20°C until required and was labeled with clinical grade ^89^Zr-oxalate on the day of use. The radiochemical purity (RCP) of [^89^Zr]-fresolimumab was 97.0 ± 1.2% as determined with high-performance liquid chromatography (HPLC), and it was used without further purification. The specific activity of the labeled mAb was reported to be up to 1,000 MBq/6.6 nmol (2.7 mCi/6.6 nmol).

[^89^Zr]-Fresolimumab was stable in 0.9% NaCl at 4°C and in human serum at 37°C for >168 h as determined with HPLC (5).

Human IgG was conjugated to 2-(4-isothiocyanatobenzyl)-diethylenetriaminepentaacetic acid and then labeled with ^111^In ([^111^In]-IgG) on the required day for use as a control in the biodistribution study (5). The radiochemical yield, RCP, specific activity, and stability of the labeled IgG were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-fresolimumab%20in%20vitro&cmd=DetailsSearch)]

In a competitive TGF-β binding assay with [^89^Zr]-fresolimumab in the presence of increasing concentrations of unlabeled fresolimumab, the 50% inhibition of the maximum binding of labeled fresolimumab was determined to be 14 nM compared with 18 nM for the unlabeled mAb (5). This indicated that conjugating the mAb with N-sucDf-TFP and labeling it with ^89^Zr did not alter the affinity of [^89^Zr]-fresolimumab for the ligand.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-fresolimumab%20rodentia&cmd=DetailsSearch)]

Two different biodistribution studies were performed with nude mice bearing either Chinese hamster ovary (CHO) cell or human breast cancer MDA-MB-231 cell subcutaneous xenograft tumors as described by Oude Munnink et al. (5).

For the CHO cell study, nude mice bore either CHO-Cl11S cell (produces intermediate levels of latent TGF-β; 23.3 ng/10^6^ cells/day; determined in the growth medium with ELISA) or CHO-C12 cell (produces high levels of latent TGF-β; 189 ng/10^6^ cells/day; determined in the growth medium with ELISA) subcutaneous xenograft tumors. The mice (n = 2–6 animals/dose) were administered [^89^Zr]-fresolimumab (5 MBq (135 μCi) in 66.6 pmol, 333 pmol, or 666 pmol mAb) or [^111^In]-IgG (3 MBq (81 μCi) in 66.6 pmol, 333 pmol, or 666 pmol IgG) through the penile vein. The animals were euthanized at 144 h postinjection (p.i.) to determine the amount of radioactivity accumulated in the various organs of the animals. Data obtained from the study were expressed as percent of injected dose per gram tissue (% ID/g). A comparable uptake of both tracers was observed in all the organs and tumors of the animals, except in the liver and bone, which showed a higher accumulation of label from [^89^Zr]-fresolimumab than from [^111^In]-IgG. Only in the kidneys and liver of mice injected with the 66.6 pmol dose was there a 92 ± 28% (P = 0.0078) and 69 ± 28% (P = 0.0005), respectively, higher uptake of the tracer from [^89^Zr]-fresolimumab than from [^111^In]-IgG. Assessment of TGF-β levels in liver homogenates with ELISA showed there was no increase in the level of the active cytokine in this organ. The investigators suggested that the higher levels of ^89^Zr observed in the liver were probably because the breakdown products of [^89^Zr]-fresolimumab had accumulated in the liver or degradation products of TGF-β from other organs that had bound [^89^Zr]-fresolimumab were present in this organ for disposal. A similar trend was observed in the tumors of mice bearing the CHO-C12 or CHO-Cl11S xenografts.

Small-animal PET images were acquired from mice bearing the CHO-Cl11S or CHO-C12 cell xenograft tumors at 24, 72, and 144 h p.i (5). No difference in the uptake of radioactivity from [^89^Zr]-fresolimumab was apparent from the PET images of the tumors from the two CHO clones. No single-photon emission computed tomography images of animals injected with [^111^In]-IgG were reported for comparison with the images obtained with [^89^Zr]-fresolimumab. In addition, hematoxylin and eosine staining showed no morphological differences between the xenograft tumors originating from either CHO clone.

In another study, the MDA-MB-231 cell human breast cancer xenograft mouse model (number of mice used for the study was not reported) was used to study the biodistribution of [^89^Zr]-fresolimumab (5 MBq (135 μCi) in 66.6 pmol/animal) and [^111^In]-IgG (3 MBq (81 μCi) in 66.6 pmol/animal) (5). The biodistribution of label from both radiolabeled immunoreagents was similar to that observed during the CHO studies mentioned above.

Because breast cancer is often metastasized to the bone, [^89^Zr]-fresolimumab was also evaluated for the visualization of bone metastasis in a mouse metastatic breast cancer model (5). The animals developed bone metastasis 3–5 weeks after intracardiac injection of MDA-MB-231-SCP2luc cells (a bone tropic clone of MDA-MB-231 cells that are transfected with a luciferase and described elsewhere (6)). The metastasis was confirmed in the animals with bioluminescence imaging (BLI) and was located mainly in the jaws, skull, sternum, spine shoulders, hips, and lower limbs of the animals. The mice were injected with [^89^Zr]-fresolimumab, and small-animal PET images were acquired as before. The investigators reported that neither micro-computed tomography nor small-animal PET could detect the metastasis visualized with BLI.

From these studies, the investigators concluded that [^89^Zr]-fresolimumab can be used with small-animal PET to visualize neoplastic tumors that express TGF-β in mice (5).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-fresolimumab%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-fresolimumab%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-fresolimumab%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Hawinkels L.J., Ten Dijke P. (2011). Exploring anti-TGF-beta therapies in cancer and fibrosis. Growth Factors.
2 Meulmeester E., Ten Dijke P. (2011). The dynamic roles of TGF-beta in cancer. J Pathol.
3 Inman G.J. (2011). Switching TGFbeta from a tumor suppressor to a tumor promoter. Curr Opin Genet Dev.
4 Garber K. (2009). Companies waver in efforts to target transforming growth factor beta in cancer. J Natl Cancer Inst.
5 Oude Munnink T.H., Arjaans M.E., Timmer-Bosscha H., Schroder C.P., Hesselink J.W., Vedelaar S.R., Walenkamp A.M., Reiss M., Gregory R.C., Lub-de Hooge M.N., de Vries E.G. (2011). PET with the 89Zr-Labeled Transforming Growth Factor-beta Antibody Fresolimumab in Tumor Models. J Nucl Med.
6 Minn A.J., Kang Y., Serganova I., Gupta G.P., Giri D.D., Doubrovin M., Ponomarev V., Gerald W.L., Blasberg R., Massague J. (2005). Distinct organ-specific metastatic potential of individual breast cancer cells and primary tumors. J Clin Invest.